# ^111^In-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-T84.66 scFv-human serum albumin

Chemical name: | ^111^In-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-T84.66 scFv-human serum albumin
Abbreviated name: | ^111^In-DOTA-T84.66 scFv-HSA
Synonym:
Agent category: | Antibody fragment
Target: | Carcinoembryonic antigen (CEA)
Target category: | Antigen
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=180211), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=29856) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=5670) for more information about CEA

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv)]

Carcinoembryonic antigen (CEA) was first identified from extracts of human colon adenocarcinoma (1) and fetal gut (2). It is a β-glycoprotein, and its predominant expression on the cell surface is increased in a variety of carcinomas and in certain inflammatory conditions such as inflammatory bowel disease (3, 4). CEA has a molecular weight of ~180 kDa, and it can be shed and detected in the serum (5). CEA expression is observed in patients with various carcinomas of the colon, lungs, thyroid, uterus, ovaries, pancreas, and medullary thyroid (6). Radiolabeled monoclonal antibodies (mAbs) have been developed for both the diagnosis and treatment of tumors (7, 8).

Single-chain variable fragments (scFvs) of mAbs with a molecular mass of 25 kDa are cleared very rapidly from the circulation, but they exhibit poor tumor retention because they have a lower affinity than the parent antibody (9). On the other hand, bivalent antibody fragments possess more ideal tumor-targeting characteristics, including rapid tissue penetration, high target retention, and rapid blood clearance. The diabody fragment (a dimer of scFvs; molecular mass = 55 kDa) and the minibody fragment (a dimer of scFvs-C_H_3 with a linker comprising 18 amino acids; molecular mass = 80 kDa) of a murine/human chimeric anti-CEA T84.66 antibody have been evaluated for targeting in several tumor antigen systems with rapid tumor localization and high-contrast imaging (9, 10). In particular, murine/human chimeric anti-CEA T84.66 diabody and minbody, which retain excellent CEA-binding properties (dissociation constant = 0.01–0.6 nM) (11-13), were developed as CEA imaging agents. However, the pharmacokinetics of radiometal labeled antibodies, with high liver and kidney uptake, are generally not ideal for imaging (14). Albumin is known to accumulate in tumors (15) and has a long blood half-life (16). Furthermore, albumin fusion proteins have been shown to prolong the in vivo circulation of small peptides and proteins (17). A T84.66 single-chain antibody (scFv) was joined with human serum albumin (HSA) using recombinant technology to form T84.66 scFv-albumin fusion protein (T84.66 scFv-HSA), which was radiolabeled with ^111^In for localization of CEA-positive tumors in mice with single-photon emission computed tomography (SPECT) (18).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv%20+and%20synthesis)]

The recombinant T84.66 scFv-HSA was conjugated with N-hydroxysuccinimidyl-DOTA in a molar ratio of 1:17 (18). The DOTA-scFv-HSA (2 nmol) was incubated with 32.56 MBq (0.88 mCi) of ^111^InCl_3_ (pH, 5.5) at 43°C for 30 min. ^111^In-DOTA-T84.66 scFv-HSA was isolated with size-exclusion chromatography with a radiolabeling efficiency of ~100%. The specific activity was ~14.8 MBq/nmol (0.4 mCi/nmol) at the end of purification.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv%20and%20in%20vitro)]

Radioimmunoreactivity of ^111^In-DOTA-T84.66 scFv-HSA for recombinant CEA was determined to be 88% with high-performance liquid chromatography analysis (18).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv+and%20rodentia)]

Yazaki et al. (18) performed biodistribution studies of ^111^In-DOTA-T84.66 scFv-HSA in nude mice (n = 5 mice/group) with the use of a LS174T human colon carcinoma subcutaneous xenograft model. Data were obtained at 0, 4, 18, 24, 48, and 72 h after injection. Accumulation of the ^111^In-DOTA-T84.66 scFv-HSA in the CEA-expressing LS174T tumor was 13.8 ± 1.5% injected dose (ID)/g at 4 h and reached a maximum level of 37.2 ± 7.0% ID/g at 18 h. The tumor/blood ratio was 18.8 at 72 h. All other major organs exhibited lower levels of radioactivity than the tumor. The liver had the highest accumulation with a plateau of 11-12% ID/g at 18-72 h. The heart, spleen, lungs, and kidneys had lower levels of radioactivity than the LS174T tumor. The rapid blood clearance pattern exhibited a two-phase model with a half-life of 1 h during the distribution phase and a half-life of 15 h during the elimination phase. ^111^In-DOTA-T84.66 scFv-HSA exhibited a markedly slower blood clearance than the T84.66 minibody and diabody but cleared faster than the parent T84.66 antibody. SPECT imaging with the ^111^In-DOTA-T84.66 scFv-HSA showed high localization to the CEA-positive tumor and relatively low activity elsewhere (except the liver) in the mice, confirming the biodistribution data. No blocking experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv+and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=T84.66%20scFv+and%20human)]

## References

1 Gold P., Freedman S.O. (1964). Demonstration of tumor-specific antigens in human colonic carcinomata by immunological tolerance and absorption techniques. The Journal of Experimental Medicine.
2 Krupey J., Gold P., Freedman S.O. (1967). Purification and characterization of carcinoembryonic antigens of the human digestive system. Nature.
3 Kowalsky, R.J., and S.W. Falen, Radiopharmaceuticals in nuclear pharmacy and nuclear medicine2004, American Pharmacists Association: Washington, D.C. p. 733-752.
4 Wahl R.L., Philpott G., Parker C.W. (1983). Monoclonal antibody radioimmunodetection of human-derived colon cancer. Invest Radiol.
5 Primus F.J., Freeman J.W., Goldenberg D.M. (1983). Immunological heterogeneity of carcinoembryonic antigen: purification from meconium of an antigen related to carcinoembryonic antigen. Cancer Res.
6 Package Insert. CEA-Scan (Arcitumomab) for the preparation of Tc 99m Arcitumomab1999, Immunomedics, Inc. p. 1-15.
7 Kenanova V., Wu A.M. (2006). Tailoring antibodies for radionuclide delivery. Expert Opin Drug Deliv.
8 Wu A.M., Senter P.D. (2005). Arming antibodies: prospects and challenges for immunoconjugates. Nat Biotechnol.
9 Wu A.M., Chen W., Raubitschek A., Williams L.E., Neumaier M., Fischer R., Hu S.Z., Odom-Maryon T., Wong J.Y., Shively J.E. (1996). Tumor localization of anti-CEA single-chain Fvs: improved targeting by non-covalent dimers. Immunotechnology.
10 Viti F., Tarli L., Giovannoni L., Zardi L., Neri D. (1999). Increased binding affinity and valence of recombinant antibody fragments lead to improved targeting of tumoral angiogenesis. Cancer Res.
11 Fagerstam L.G., Frostell-Karlsson A., Karlsson R., Persson B., Ronnberg I. (1992). Biospecific interaction analysis using surface plasmon resonance detection applied to kinetic, binding site and concentration analysis. J Chromatogr.
12 Hefta L.J., Neumaier M., Shively J.E. (1998). Kinetic and affinity constants of epitope specific anti-carcinoembryonic antigen (CEA) monoclonal antibodies for CEA and engineered CEA domain constructs. Immunotechnology.
13 Williams L.E., Wu A.M., Yazaki P.J., Liu A., Raubitschek A.A., Shively J.E., Wong J.Y. (2001). Numerical selection of optimal tumor imaging agents with application to engineered antibodies. Cancer Biother Radiopharm.
14 Yazaki P.J., Wu A.M., Tsai S.W., Williams L.E., Ikler D.N., Wong J.Y., Shively J.E., Raubitschek A.A. (2001). Tumor targeting of radiometal labeled anti-CEA recombinant T84.66 diabody and t84.66 minibody: comparison to radioiodinated fragments. Bioconjug Chem.
15 Wang J., Ueno H., Masuko T., Hashimoto Y. (1994). Binding of serum albumin on tumor cells and characterization of the albumin binding protein. J Biochem.
16 Dennis M.S., Zhang M., Meng Y.G., Kadkhodayan M., Kirchhofer D., Combs D., Damico L.A. (2002). Albumin binding as a general strategy for improving the pharmacokinetics of proteins. J Biol Chem.
17 Dennis M.S., Jin H., Dugger D., Yang R., McFarland L., Ogasawara A., Williams S., Cole M.J., Ross S., Schwall R. (2007). Imaging tumors with an albumin-binding Fab, a novel tumor-targeting agent. Cancer Res.
18 Yazaki P.J., Kassa T., Cheung C.W., Crow D.M., Sherman M.A., Bading J.R., Anderson A.L., Colcher D., Raubitschek A. (2008). Biodistribution and tumor imaging of an anti-CEA single-chain antibody-albumin fusion protein. Nucl Med Biol.